# NRluc-hER_281-549_-CRluc

Chemical name: | NRluc-hER_281-549_-CRluc
Abbreviated name: | hERNCRluc
Synonym:
Agent category: | Polypeptide
Target: | Other
Target category: | Other - protein folding
Method of detection: | Optical imaging
Source of signal/contrast: | Luciferin
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hER + split Renilla luciferase)]

Estrogen receptors (ERs) are ligand-inducible nuclear transcription factors belonging to the superfamily of steroid hormone receptors (1). The endogenous ligands of ERs such as estradiol (E2) (2), an important estrogen in humans, are secreted by endocrine cells and distributed to their targets via blood circulation (3). Upon the binding of estrogens to their inactive apoprotein forms in the cytoplasm or nucleus, ERs are transformed into active receptors that can effectively bind to a DNA element (hormone response element, HRE), leading to transcription of genes (3). ERs consist of six functional domains (A–F): the A/B region contains transactivation functions, region C contains DNA-binding domain (DBD), and region E contains ligand-binding domain (LBD) with an activation function (AF-2) (4). The LBD is an antiparallel helical sandwich of three layers formed by twelve α-helices (H1–H12) and one β-turn (5). The helix H12 serves as a lid in the ligand-binding cavity, thus, behaves as a “molecular switch” to prevent or enhance ER from binding to an array of co-activator proteins (6). The binding of ligands induces a reposition of the helices, especially the reorientation of H12, in the LBD, and can generate different functions. For instance, the binding of ER agonists such as E2 or diethylstilbestrol (DES) leads to H12 aligned over the LBD to yield a specific binding site for the consensus LXXLL motif in AF-2; the binding of selective ER modulators (SERMs) such as raloxifene or tamoxifen sterically hinders the H12 positioning to prevent the formation of a binding surface for AF-2 (4). ERs are responsible for the growth, development, and maintenance of the reproductive skeletal, neuronal, and immune systems (6). The deficiency or excess of estrogens can lead to various diseases including osteoporosis and breast carcinoma. A variety of therapeutic strategies have been developed on the basis of the anti-ER mechanism, including the use of SERMs to provide optimal agonist or antagonist activities in ER-expressed tissues.

Renilla luciferase (Rluc) is a 36-kDa enzyme protein extracted from a bioluminescent soft coral (sea pansy (Renilla reniformis)) (7). Rluc can catalyze emission of light from substrates; i.e., the oxidation of coelenterazine to coelenteramide generates a green fluorescence (535–550 nm) (8). Rluc can be split into two domains: a large N-terminal domain (amino acids 1–221) and a C-terminal domain (amino acids 230–311) (9). Splitting Rluc into N- and C-terminal fragments destroys its enzymatic activity, resulting in a complete loss of bioluminescence. The enzymatic activity or bioluminescence can be restored if the N- and C-terminal fragments are in close proximity. This led to the development of the split reporter, a novel labeling strategy that has been used in imaging protein–protein interactions (10) and/or protein activity (11) in vivo. For instance, protein A is connected with the N-terminal fragment of Rluc, and protein B is connected with the C-terminal fragment of Rluc. Interaction between proteins A and B recovers the enzymatic activity of Rluc by bringing the two fragments of Rluc close together, which allows for recovery of bioluminescence (10).

NRluc-hER_281-549_-CRluc (hERNCRluc) is an optical agent used to image the intramolecular folding of human ER (hER) in vivo (6). hERNCRluc consists of four sequentially linked components: an N-terminal Rluc (N-Rluc) fragment, a fragment of hER α-isoform (hERα) containing the LBD (amino acids 281–549, hER_281-549_), a spacer linker ((GGGGS)_2_), and a C-terminal Rluc (C-Rluc). The included hER fragment (hER_281-549_) provides a binding cavity for various ligands, and its conformation can be altered upon binding of the ligands. Depending on the produced protein-folding pattern, partial to full complementation of the N-Rluc and C-Rluc occurs, which is measurable with bioluminescence imaging. hERNCRluc is suitable for distinguishing the functionalities in various ER ligands (i.e., agonists, antagonist, or SERMs) with in vivo imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( hER + split Renilla luciferase)+AND+synthesis%0D%0A)]

Paulmurugan et al. briefly described the preparation of hERNCRluc via complementation strategy (6, 10). The N-terminal portion (amino acids 1–229) was amplified with polymerase chain reaction (PCR) using Nhel forward primer with start codon and BamHI reverse primer with the peptide linker sequence (GGGGS)_2_ with phRL-CMV as a template. The C-terminal portion (amino acids 230–311) of the Rluc gene was also amplified with PCR using BamHI forward primer and Xhol reverse primer with stop codon. The fragments were cloned into the Nhel and Xhol restriction sites pcDNA3.1(+) to generate the plasmid vector pcDNA-NRluc-CRluc. Then the fragment (amino acids 281–549) of hERα gene was amplified with PCR using BamHI forward primer and BamHI reverse primer followed by subsequent insertion into the plasmid vector pcDNA-NRluc-CRluc. The produced pcDNA-NRluc-hER_281-549_-CRluc plasmids were used to transfect 293T cells (ER-negative) using lipofectamine, where the fusion protein, NRluc-hER_281-549_-Rluc, was expressed.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( hER + split Renilla luciferase)+AND+%22in+vitro%22)]

Paulmurugan et al. used hERNCRluc to examine the ligand-induced hER intramolecular folding in vitro (6). 293T cells were transiently transfected with pcDNA-NRluc-hER_281-549_-CRluc. Before and after treatment with 1 μM of various ER ligands, Rluc protein activity was assayed to measure its complementation level, and the complemented Rluc protein level was evaluated with Western blot analysis. Compared with the control (DMSO), the complementation level was found to increase 80-fold ± 15-fold with ER SERMs (tamoxifen, raloxifene, 4-hydroxytamoxifen (4-OHT)), 15-fold ± 5 fold with ER agonists (E2, DES), and no apparent complementation with a very low affinity ER agonist genistein. The treatment with E2, DES, genistein, and raloxifene caused little change in the Rluc level, but a significant reduction was found in the cells treated with the SERM tamoxifen. These results demonstrated that the variations in Rluc activity were not mediated through the Rluc protein level but were more likely to be caused by different complementation patterns within the receptor induced by the ligands. To reduce the binding of endogenous agonist E2, a mutant hERα segment with a glycine-to-threonine (G521T) transition (hER_281-549/G521T_) was studied under the similar conditions. 293T cells were transiently transfected with pcDNA-NRluc-hER_281-549(G521T)_-CRluc followed by treatment with 1 μM of the agonists or SERMs. The threonine replacement of Gly521 led to a 94% reduction in the E2-induced Rluc activity, a 12–22% reduction in Rluc activity induced by DES, 4-OHT, or raloxifene, and no significant change in Rluc activity after genistein treatment. The results suggested that the mutant hER retained much higher sensitivity to DES and the SERMs compared with the endogenous agonist E2, which allows the in vivo evaluation of the effects of various ligands. Paulmurugan et al. also studied the kinetics of ligand-induced Rluc complementation in vitro (6). 293T cells were transiently transfected with pcDNA-NRluc-hER_281-549_-CRluc and subsequently treated with 1 μM of agonists (E2, DES) or SERM (4-OHT). The cells were assayed for the Rluc activity at 6, 12, 18, and 24 h after treatment. All treated cells exhibited increased Rluc activity compared with the control (DMSO), and the activity in 4-OHT–treated cells was significantly higher than that in cells treated with E2 or DES at all time points.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( hER + split Renilla luciferase) +AND++rodentia)]

Paulmurugan et al. used hERNCRluc to examine the ligand-induced hER intramolecular folding in vivo (6). 293T cells that were stably transfected with pcDNA-NRluc-hER_281-549_-CRluc (expressing wild-type hER, the wild-type hER sensor) or pcDNA-NRluc-hER_281-549(G521T)_-CRluc (expressing mutant hER, the mutant hER sensor) were implanted in the lower backs of nude female mice (n = 3). Bioluminescence imaging of Rluc activity was performed with a cold charged-coupled device (CCD) camera immediately after cell implantation and 18 h after intraperitoneal injection of raloxifene (0.5 mg). In each imaging session, 100 μl coelenterazine (50 μg) in PBS was injected intravenously into mice at 5 s before imaging. A significantly higher Rluc activity was observed at the site with the mutant hER sensor (9.7 ± 1.2 × 10^3^ photons per second per square centimeter per steradian (p/s/cm^2^/sr)) than at the site with the wild-type hER sensor (2.16 ± 0.52 × 10^3^ p/s/cm^2^/sr). The low Rluc activity in the wild-type hER sensor was most likely related to the competitive binding of endogenous agonist E2 in the animal. In a similar manner, the mutant hER sensor was used to differentiate ER ligands with in vivo imaging. Bioluminescence images were collected 24 h after the implantation of transfected cells (before ligand administration) and every 24 h after administration of 24 μg of ER agonist (DES) or SERM (4-OHT) in sesame oil or 50 μl sesame oil as a control. A significantly higher Rluc activity was observed in the animal that received the SERM (4-OHT) (~2.2 × 10^3^ p/s/cm^2^/sr) than in the animal that received the agonist (DES) or that served as the control (~1 × 10^3^ p/s/cm^2^/sr) at 48 h, demonstrating the feasibility to distinguish ER ligand in living animals.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( hER + split Renilla luciferase) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( hER + split Renilla luciferase) +AND+human)]

No publication is currently available.

### NIH Support

CA114747, CA92865, CA82114

## References

1 Brzozowski A.M., Pike A.C., Dauter Z., Hubbard R.E., Bonn T., Engstrom O., Ohman L., Greene G.L., Gustafsson J.A., Carlquist M. (1997). Molecular basis of agonism and antagonism in the oestrogen receptor. Nature.
2 Pike A.C., Brzozowski A.M., Walton J., Hubbard R.E., Bonn T., Gustafsson J.A., Carlquist M. (2000). Structural aspects of agonism and antagonism in the oestrogen receptor. Biochem Soc Trans.
3 Tsai M.J., O'Malley B.W. (1994). Molecular mechanisms of action of steroid/thyroid receptor superfamily members. Annu Rev Biochem.
4 Shao W., Brown M. (2004). Advances in estrogen receptor biology: prospects for improvements in targeted breast cancer therapy. Breast Cancer Res.
5 Moras D., Gronemeyer H. (1998). The nuclear receptor ligand-binding domain: structure and function. Curr Opin Cell Biol.
6 Paulmurugan R., Gambhir S.S. (2006). An intramolecular folding sensor for imaging estrogen receptor-ligand interactions. Proc Natl Acad Sci U S A.
7 Venisnik K.M., Olafsen T., Loening A.M., Iyer M., Gambhir S.S., Wu A.M. (2006). Bifunctional antibody-Renilla luciferase fusion protein for in vivo optical detection of tumors. Protein Eng Des Sel.
8 Loening A.M., Wu A.M., Gambhir S.S. (2007). Red-shifted Renilla reniformis luciferase variants for imaging in living subjects. Nat Methods.
9 Paulmurugan R., Gambhir S.S. (2003). Monitoring protein-protein interactions using split synthetic renilla luciferase protein-fragment-assisted complementation. Anal Chem.
10 Paulmurugan R., Massoud T.F., Huang J., Gambhir S.S. (2004). Molecular imaging of drug-modulated protein-protein interactions in living subjects. Cancer Res.
11 Zhang L., Lee K.C., Bhojani M.S., Khan A.P., Shilman A., Holland E.C., Ross B.D., Rehemtulla A. (2007). Molecular imaging of Akt kinase activity. Nat Med.